# Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid monoamide-G2 nanoglobule-CGLIIQKNEC (CLT1)-Cy5

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid monoamide-G2 nanoglobule-CGLIIQKNEC (CLT1)-Cy5
Abbreviated name: | CLT1-G2-(Gd-DOTA-MA)-Cy5
Synonym:
Agent category: | Peptide
Target: | Fibrin-fibronectin clot complexes
Target category: | Acceptor
Method of detection: | Multimodal: magnetic resonance imaging (MRI); near-infrared (NIR) fluorescence imaging, optical
Source of signal/contrast: | Gadolinium, Gd; Cy5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1)]

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). A meshwork of clotted plasma protein is present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (3). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (4, 5). Gd-Diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent to be used in the clinic, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and tumor tissues (6). Furthermore, these agents are largely nonspecific. CGLIIQKNEC (CLT1), a fibronectin-fibrin–binding cyclic peptide, was identified with phage display screening (3). The peptide was conjugated with Gd-DTPA to form Gd-DTPA-CLT1 for use with imaging of fibronectin-fibrin complexes in tumor tissues, and this agent exhibited specific accumulation in the tumors (7). Tan et al. (8) prepared Gd-DOTA-G3-CLT1, a CLT1-targeted contrast agent with Gd-tetraazacyclododecane-1,4,7,10-tetraacetic acid (GD-DOTA)_43_ monoamide chelates and three CLT1 molecules conjugated to a generation 3 (G3) polylysine dendrimer with a cubic silsesquioxane core. Gd-DOTA-G3-CLT1 was evaluated as a MRI tumor contrast agent in nude mice bearing MDA-MB-231 human breast carcinoma xenografts. Subsequently, Tan et al. (9) prepared CLT1-G2-(Gd-DOTA-MA)-Cy5, a CLT1-targeted G2 nanoglobular Gd-DOTA monoamide and Cy5 conjugate for use with multimodality (MRI and optical) imaging of prostate cancer.

### Related Resource Links:

- Chapters in MICAD (CLT1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CLT1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), fibronectin (http://omim.org/entry/135600))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+synthesis)]

The CLT1 conjugate with a polyethylene glycol (PEG)-propargyl group at the N-terminus was synthesized using solid-phase peptide synthesis (9). The G2 nanoglobules were synthesized as previously described (10) and activated with azido-PEG N-hydroxysuccinimide for CTL1 conjugation and DOTA-tris(t-Bu) for labeling with Gd (9). The G2 nanoglobule-(DOTA)_20_-(Lys-PEG-azido)_3_ conjugate was prepared with 70% yield, and its molecular weight was confirmed with mass spectroscopy. The G2 nanoglobule-(DOTA)_20_-(Lys-PEG-azido)_3_ conjugate (10.8 µmol) was incubated with excess Gd(OAc)_3_ for 6 d at room temperature. The product, G2 nanoglobule-(Gd-DOTA)_20_-(Lys-PEG-azido)_3_ conjugate, was purified with column chromatography with 64% yield. The G2 nanoglobule-(Gd-DOTA)_20_-(Lys-PEG-azido)_3_ conjugate (2 µmol) was incubated with Cy5-NHS ester (7.2 µmol) for 24 h at room temperature to conjugate Cy5 to the ε-amino group of the (Lys-PEG-azido)_3_ linkers. The G2 nanoglobule-(Gd-DOTA)_20_-(PEG-azido)_3_-Cy5 conjugate was purified with ultrafiltration with 87% yield. The G2 nanoglobule-(Gd-DOTA)_20_-(PEG-azido)_3_-Cy5 conjugate (2 µmol), copper(II) sulfate (2 µmol), and CTL1-PEG-propargyl conjugate (16 µmol) were incubated for 40 h at room temperature. The final product, (CTL1)_3_-G2 nanoglobule-(Gd-DOTA)_20_-Cy5_1_ (CLT1-G2-(Gd-DOTA-MA)-Cy5) conjugate, was purified with ultrafiltration and dialysis with 33% yield, and its molecular weight (30.3 kDa) was confirmed with mass spectroscopy. The control peptide, KAREC-modified G2 nanoglobule (KAREC-G2-(Gd-DOTA-MA)-Cy5) (29.9 kDa), was similarly prepared. There were twenty Gd, one Cy5, and three peptide moieties per G2 nanoglobule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+in+vitro)]

CLT1-G2-(Gd-DOTA-MA)-Cy5 exhibited r_1_ and r_2_ values of 13.4 mM^–1^s^–1^ per Gd and 14.6 mM^–1^s^–1^ per Gd at 1.5 T (9), respectively. Non-targeted KAREC-G2-(Gd-DOTA-MA)-Cy5 exhibited r_1_ and r_2_ values of 12.2 mM^–1^s^–1^ per Gd and 13.9 mM^–1^s^–1^ per Gd at 1.5 T, respectively. Both conjugates had the same fluorescence spectra as Cy5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+rodentia)]

Tan et al. (9) performed dynamic T1-weighted MRI (7 T) studies with intravenous injection of 0.03 mmol Gd/kg CLT1-G2-(Gd-DOTA-MA)-Cy5 or KAREC-G2-(Gd-DOTA-MA)-Cy5 in nude mice (n = 4/group) bearing orthotopic PC3 human prostate tumors. Contrast-enhanced MRI images were obtained before injection and at 1, 5, 10, 15, 20, 25, 30, 35, and 40 min after injection. Enhanced contrast in the tumor tissues was visualized for CLT1-G2-(Gd-DOTA-MA)-Cy5 at 1–40 min after injection. Contrast/noise ratios (CNRs) were 16, 17, 16, 14, and 13 at 1, 5, 10, 30, and 40 min after injection, respectively. The tumor CNRs for non-targeted KAREC-G2-(Gd-DOTA-MA)-Cy5 were significantly lower than those for CLT1-G2-(Gd-DOTA-MA)-Cy5 (P < 0.05), ranging from 6 at 1 min to 8 at 40 min. Ex vivo fluorescence imaging was performed at 2 h after injection of CLT1-G2-(Gd-DOTA-MA)-Cy5 in nude mice bearing orthotopic PC3 human prostate tumors. The tumor and lung were clearly visualized, and little fluorescence intensity was observed in the other organs. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+human)]

No publication is currently available.

## NIH Support

R01 CA097465

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
4 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
5 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
6 Laurent S., Elst L.V., Muller R.N. (2006). Comparative study of the physicochemical properties of six clinical low molecular weight gadolinium contrast agents. Contrast Media Mol Imaging.
7 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
8 Tan M., Wu X., Jeong E.K., Chen Q., Lu Z.R. (2010). Peptide-targeted Nanoglobular Gd-DOTA monoamide conjugates for magnetic resonance cancer molecular imaging. Biomacromolecules.
9 Tan, M., Z. Ye, D. Lindner, S.M. Brady-Kalnay, and Z.R. Lu, Synthesis and Evaluation of a Targeted Nanoglobular Dual-Modal Imaging Agent for MR Imaging and Image-Guided Surgery of Prostate Cancer. Pharm Res, 2013
10 Kaneshiro T.L., Jeong E.K., Morrell G., Parker D.L., Lu Z.R. (2008). Synthesis and evaluation of globular Gd-DOTA-monoamide conjugates with precisely controlled nanosizes for magnetic resonance angiography. Biomacromolecules.